# ZW800-1, a zwitterionic near-infrared fluorophore, and its cyclic RGD peptide derivative cyclo-(RGDyK)-ZW800-1

Chemical name: | ZW800-1, a zwitterionic near-infrared fluorophore, and its cyclic RGD peptide derivative cyclo-(RGDyK)-ZW800-1
Abbreviated name: | ZW800-1 and cRGD-ZW800-1
Synonym:
Agent Category: | Compound
Target: | Non-targeted (ZW800-1); integrin α_v_β_3_ (cRGD-ZW800-1)
Target Category: | Non-targeted (ZW800-1); receptor (cRGD-ZW800-1)
Method of detection: | Optical imaging (near-infrared fluorescence (NIRF) imaging)
Source of signal / contrast: | ZW800-1
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5bAll%20Fields%5d&cmd=DetailsSearch)]

Indocyanine green (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=b3d23a29-6413-4fe0-96ec-858d15659aa2) (ICG) is a noninvasive near-infrared (NIR) fluorescence (NIRF) imaging dye that is approved by the United States Food and Drug Administration (FDA) for ophthalmic angiography to determine cardiac output and liver blood flow and function. This dye is also used in cancer patients to map sentinel lymph nodes (SLN), for the detection of solid tumors, and for angiography during reconstructive surgery (2). Methylene blue (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=04cea07f-f3f0-4c45-9f56-67dc8ebe7ddf) (MB) is another NIRF dye that has been approved by the FDA for the treatment of drug-induced methemoglobinemia (http://www.nlm.nih.gov/medlineplus/ency/article/000562.htm), but MB is also used to visualize SLNs with ultrasound imaging in the clinic (3). Two other commercially available NIRF dyes, Cy5.5 and IRDye800-CW (CW800), have been coupled with peptides or antibodies and successfully used for the targeted visualization of neoplastic tumors in rodents (4). Although the NIRF dyes exhibit low autofluorescence, tissue absorbance, and scatter at NIR wavelengths (700–900 nm), a major limitation of using these dyes in the clinic is that they often show high nonspecific binding and have high tissue uptake and retention (5). In addition, these dyes are cleared from circulation primarily through the hepatobiliary pathway and generate high background signals in the gastrointestinal tract, which results in the masking of signals from cancerous lesions that may be present in tissues located around the digestive system (5). The high background signals interfere with distinguishing the tumors from normal tissues during NIRF-guided resection of the lesions (6). Physiochemical properties such as positive/negative charge density, charge distribution, and hydrophilicity/hydrophobicity (or lipophilicity) are known to affect the protein binding, serum stability, and in vivo biodistribution characteristics of compounds and imaging agents, including probes of the NIRF variety (7). In this regard, MB carries a small net positive charge (+1), whereas ICG, Cy5.5, and CW800 carry a net negative charge (−1, −4, and −4, respectively) and are hydrophobic (Table 1) (6). The physiochemical properties of these NIRF dyes are discussed in detail by Gioux et al. (6).

Results obtained from a biodistribution study of NIRF nanoparticles (NPs) with different chemical compositions, hydrodynamic diameters, shapes, and surface charges administered to rats through the pulmonary route showed that zwitterionic NPs (i.e., NPs with a net zero charge or charge-neutral), compared with cationic or anionic charged NPs, were rapidly absorbed from the lungs and were moved to the SLN and into blood circulation for clearance through the kidneys (8). Similar results were reported with zwitterionic quantum dots (QDs) conjugated to CW800 and decorated with a limited number of small molecule (2-(3-amino-3-carboxypropyl)) or peptide (cyclo-RGD-yK) ligands that targeted the prostate-specific membrane antigen and the α_v_β_3_ integrin receptor, respectively (9). On the basis of these studies, it was hypothesized that NIRF agents with a net zwitterionic charge would probably behave in a manner similar to the zwitterionic NPs and QDs under in vivo conditions (7). In addition, it was expected that the charge-neutral NIRF agents would generate superior images compared with NIRF probes that carried a net anionic or cationic charge. To test this hypothesis, the biodistribution of a series of heptamethine indocyanine NIRF probes with varying net charges, e.g., ICG (net charge −1), CW800 (net charge −4), RS800 (a derivative of CW800, net charge −2), ZW800-1 (a derivative of CW800, net charge 0), and ZW800-3a (a derivative of CW800, net charge +2) was investigated in mice (7). In another study, cyclo-(RGDyK) conjugated to ZW800-1 (cRGD-ZW800-1) was compared with cyclo-(RGDyK) conjugated to CW800 (cRGD-CW800) and cyclo-(RGDyK) conjugated to Cy5.5 (cRGD-Cy5.5) for the visualization of xenograft tumors that overexpressed integrin α_v_β_3_ receptors in mice (5). In addition, fibrinogen (FBG) labeled with the NIRF dyes (FBG-ZW800, FBG-CW800, and FBG-Cy5.5, respectively) was evaluated for the detection of fibrinogen-positive thrombi (blood clots) in mice (5).

### Related Resource Links

Other NIRF imaging agent chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=%28NIRF%5bAll%20Fields%5d%20AND%20imaging%5bAll%20Fields%5d%29%20AND%20micad%5bbook%5d&cmd=DetailsSearch)

Integrin-related (http://www.ncbi.nlm.nih.gov/books/?term=Integrins+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Fibrinogen (http://www.ncbi.nlm.nih.gov/books/?term=fibrinogen+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)-related chapters in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Near-infrared+fluorescence+dyes&Search=Search) involving NIRF dyes

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5bAll%20Fields%5d%20AND%20%28%22metabolism%22%5bMeSH%20Terms%5d%20OR%20%22metabolism%22%5bAll%20Fields%5d%20OR%20%22synthesis%22%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

The synthesis of ZW800-1 and ZW800-3a is described elsewhere (7). The chemical yields and chemical purities of ZW800-1 and ZW800-3a were reported to be >85% and 92%, and 97.1% and 98.7%, respectively (7).

ZW800-1 was also synthesized on a preparative scale using current good manufacturing practice (cGMP) procedures (10). With this method, the final yield of the NIRF dye was >90%, with a purity of >99%, as determined with fluorescence and evaporative light scatter detection.

In another publication, ZW800-1 was synthesized on a preparative scale synthesis, and the chemical yield of the dye was reported to be >85% (5). The final preparation of ZW800-1 had a purity of >98% as determined with analytical reverse-phased high-performance liquid chromatography and matrix-assisted laser desorption ionization time-of-flight (MALDI-TOF) mass spectrometry (MS) (5). N-Hydroxysuccinimide (NHS) esters of ZW800-1 (ZW800-1 NHS ester), CW800 (CW800 NHS ester), and Cy5.5 (Cy5.5 NHS ester) were prepared for conjugation with cRGD or FBG as described by Choi et al. (5). The purity and chemical structures of all the NIRF dye esters and the NIRF dye conjugates of cRGD or FBG were confirmed with liquid chromatography-MS and MALDI-TOF MS, respectively (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5bAll%20Fields%5d%20AND%20vitro%5bAll%20Fields%5d%20AND%20studies%5bAll%20Fields%5d&cmd=DetailsSearch)]

The fluorescence signal with 1 mg ZW800-1 in 50 mM HEPES buffer (pH 7.4) was reported to be ~3.3-fold higher than the signal with the same amount of ICG under the same conditions (10). This indicated that smaller doses of ZW800-1, compared with those of ICG, can probably be used for the different preclinical and clinical studies.

MS analysis of urine obtained from mice or pigs injected intravenously with ZW800-1 showed that the dye was excreted unchanged from both animal species (10).

The binding specificity of cRGD-ZW800-1, cRGD-CW800, and cRGD-Cy5.5 was investigated in in vitro assays with M21 cells (human melanoma cell line that expresses integrin α_v_β_3_) and M21-L cells (negative controls; do not express integrin α_v_β_3_) (5). High background fluorescence signals due to nonspecific binding of the dye were obtained in both cell lines with cRGD-CW800 and cRGD-Cy5.5, but no background signals were observed in cells exposed to cRGD-ZW800-1. To confirm these observations, the NIRF dyes were conjugated to an anti-epidermal growth factor receptor 2 antibody (anti-HER2 Ab), and MDA-MB-231 (http://atcc.org/Products/All/HTB-26.aspx) cells that overexpress the HER2 receptor were exposed to the Ab-NIRF conjugates (5). Although all three conjugates showed specific binding to the HER2-positive MDA-MB-231 cells, a high background signal was observed with the CW800 and Cy5.5 conjugates, even in the control MDA-MB-231 cells that did not express HER2. In addition, the anti-HER2 Ab-Cy5.5 conjugate showed strong nonspecific binding to both cell lines (5). No blocking studies were reported.

When the NIRF dyes were conjugated with secondary Abs and used for immunohistochemical and Western blot analysis of human prostate or breast cancer tissue samples (for a detailed description of these studies, see Choi et al. (5)), it was observed that the zwitterionic ZW800-1 Ab conjugates generated no or very little background signal compared with the anionic CW800 or Cy5.5 Ab conjugates. This again showed that the anionic dyes generated higher background signals compared with the zwitterionic NIRF dyes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5bAll%20Fields%5d%20AND%20%28%22rodentia%22%5bMeSH%20Terms%5d%20OR%20%22rodentia%22%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

The biodistribution of CW800, RS800, ICG, ZW800-1, and ZW800-3a was investigated in CD-1 mice (http://www.criver.com/en-us/prodserv/bytype/resmodover/resmod/pages/cd-1mouse.aspx) and Sprague-Dawley rats (http://www.criver.com/en-us/prodserv/bytype/resmodover/resmod/pages/spraguedawleyrat.aspx) (7). The animals (n = 6 animals/NIRF dye) were intravenously injected with 40 pmol dye/g body weight (BW), and the abdominal organs and tissues were surgically exposed at 4 h postinjection (p.i.) for fluorescence imaging. The amount of dye accumulated in the various organs of the mice and rats is presented as contrast/background ratios (CBR; defined as difference of the fluorescence signal minus the system background, with the difference divided by the system background) in Table 2. Only ZW800-1 was excreted primarily through the kidneys of both rodent species. All the cationic or anionic NIRF dyes showed a high uptake in different organs; all these agents were secreted into the bile and exhibited high fluorescence in the gastrointestinal tract of the animals. The blood circulation half-lives of the NIRF agents in the rodents were reported to be ICG>RS800>ZW800-1>CW800>ZW800-3a (7).

The biodistribution of ZW800-1 manufactured under cGMP conditions was investigated in normal CD-1 mice (10). The mice (n = 3 animals/dose) were intravenously injected with three different doses (30 nmol, 60 nmol, and 120 nmol/mouse) of the dye, and the abdominal organs and tissues were surgically exposed at 4 h p.i. for NIRF imaging. The images showed there was very low uptake of the dye in all the tissues. As discussed above (7), ZW800-1 was excreted primarily through the renal route (61.3 ± 2.15% ID/g) in all the animals, even at the maximum dose (10).

The use of cRGD-ZW800-1, cRGD-CW800, and cRGD-Cy5.5 was evaluated for the visualization of xenograft tumors generated with M21 cells (α_v_β_3_-positive) and M21-L cells (α_v_β_3_-negative) in mice (5). The animals (n = 5 mice/NIRF conjugate) were injected intravenously with 3 nmol (100 pmol/g BW) cRGD-ZW800-1 or cRGD-CW800 and 10 pmol (500 pmol/g BW) cRGD-Cy5.5, and NIRF images of the animals were acquired at 4 h p.i. Subsequently the CBR, the tumor/background ratios (TBR; defined as CBR of tumor/CBR of surrounding normal tissues), and the positive/negative tumor ratios (PNR; calculated as CBR of receptor positive tumor/CBR of receptor negative tumor) were calculated from the images (Table 3). Data in Table 3 shows that cRGD-ZW800-1 had higher TBR, CBR, and PNR compared with either cRGD-CW800 or cRGD-Cy5.5 up to 24 h p.i. This was primarily because the background signals in the normal tissues and the receptor-negative tumors were higher with cRGD-CW800 and cRGD-Cy5.5 than with cRGD-ZW800-1. The cRGD-NIRF conjugates were also evaluated for the visualization of metastatic tumors in the liver and lungs of mice (5). Although each NIRF dye was observed to accumulate in the hepatic tumors of the animals, only ZW800-1 generated a very low background, not only in this tissue, but in all the other organs also. In comparison, cRGD-CW800 and cRGD-Cy5.5 showed a high background with almost all tissues, including the liver.

During surgery, bleeding can occur in the gastrointestinal tract, and it is important to repair the damaged blood vessels to stop the bleeding. However, it may not be easy to detect the exact location of bleeding in the injured tissue. Therefore, the use of FBG-ZW800, FBG-CW800, and FBG-Cy5.5 was evaluated to detect intraoperative blood clots (thrombi, which are fibrinogen-positive) in the stomach and mesenteric vessels of rats (5). For this study, 1 h after mucosal resection in the stomach or mesenteric vessels, groups of mice (number of animals/group not reported) were injected intravenously with FBG-NIRF (40 pmol/g BW). Fluorescence intensities generated by the targeted FBG-NIRF conjugates were similar at the site of thrombosis in all the animal groups, but a marked difference was observed in the background signal intensity observed with each conjugate. At 60 min p.i., the CBRs of FBG-ZW800-1 at the mucosal and mesenteric thrombus sites were ~3.5 and ~4, respectively. At this time point, the CBRs for the mucosal and mesenteric thrombi with FBG-CW800 and FBG-Cy5.5 were ~1.9 and ~1, and ~1 and ~0.5, respectively. The higher CBRs obtained with FBG-ZW800-1 were attributed to the lower background generated by this NIRF conjugate compared with the CW800 and Cy5.5 derivatives.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5BAll%20Fields%5D%20AND%20Other%5BAll%20Fields%5D%20AND%20Non-Primate%5BAll%20Fields%5D%20AND%20Mammals%5BAll%20Fields%5D&cmd=DetailsSearch)]

The biodistribution of ZW800-1 manufactured under cGMP conditions was compared with that of ICG in normal Yorkshire pigs (10). The animals (n = 3 pigs/group) were injected intravenously with different doses of either ZW800-1 (1.2–12 μmol) or ICG (1.5–15 μmol). Subsequently, NIRF images of the surgically exposed organs/tissues of the pigs were acquired at 1 h p.i. Blood half-lives of ZW800-1 and ICG in the animals were 3.7 min and 17.9 min, respectively. The majority of the ZW800-1 was excreted through the renal system of the pigs at all doses (81.9 ± 10.7% ID for the1.2-μmol dose and 56.7 ± 10.3% ID for the 12-μmol dose). In contrast, ICG was detected in the urinary bladder only after 4 h p.i. Compared with ICG, no uptake of ZW800-1 was observed in other organs/tissues of the animals.

With results obtained from the above studies, the investigators concluded that ZW800-1 is probably superior for use with NIRF imaging compared with either CW800 or Cy5.5 (5). The investigators also mentioned that ZW800-1 has been identified as a first-in-class molecule by the United States National Cancer Institute’s Experimental Therapeutics Program for rapid translation into human clinical studies however, they do not mention weather ZW800-1 will be evaluated for the visualization of SNL or for the visualization of tumors during surgical resection (7).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5BAll%20Fields%5D%20AND%20non-human%5BAll%20Fields%5D%20AND%20primates%5BAll%20Fields%5D&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZW800-1%5BAll%20Fields%5D%20AND%20human%5BAll%20Fields%5D%20AND%20studies%5BAll%20Fields%5D&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies were supported by grants from the National Institutes of Health as follows: NCI BRP grant R01-CA-115296, NIBIB grant R01-EB-010022, and NIBIB grant R01-EB-011523.

## References

1 Slavicek J.M., Hayes-Plazolles N. (2003). The Lymantria dispar nucleopolyhedrovirus contains the capsid-associated p24 protein gene. Virus Genes.
2 Schaafsma B.E., et al. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
3 Chopra, A., [7-(dimethylamino)phenothiazin-3-ylidene]-dimethylazanium chloride Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
4 Te Velde E.A., et al. (2010). The use of fluorescent dyes and probes in surgical oncology. Eur J Surg Oncol.
5 Choi H.S., et al. (2013). Targeted zwitterionic near-infrared fluorophores for improved optical imaging. Nat Biotechnol.
6 Gioux S., Choi H.S., Frangioni J.V. (2010). Image-guided surgery using invisible near-infrared light: fundamentals of clinical translation. Mol Imaging.
7 Choi H.S., et al. (2011). Synthesis and in vivo fate of zwitterionic near-infrared fluorophores. Angew Chem Int Ed Engl.
8 Choi H.S., et al. (2010). Rapid translocation of nanoparticles from the lung airspaces to the body. Nat Biotechnol.
9 Choi H.S., et al. (2010). Design considerations for tumour-targeted nanoparticles. Nat Nanotechnol.
10 Hyun H., et al. (2012). cGMP-Compatible preparative scale synthesis of near-infrared fluorophores. Contrast Media Mol Imaging.

Table 1: Physiochemical properties of MB, ICG, Cy5.5, IRDye800-CW, and ZW800-1 NIRF dyes.

Dye | Molecular weight (Da) | Log D (at pH 7.4) | Net charge | Absorption (nm) | Emission (nm) | Quantum yield (%) | Primary clearance route
Dye | Molecular weight (Da) | Log D (at pH 7.4) | Net charge | Absorption (nm) | Emission (nm) | Quantum yield (%) | Renal | Hepatic
MB | 320 | −0.2 | +1 | 670 | 690 | 3.8 | + | ++
ICG | 775 | 7.88 | −1 | 807 | 822 | 9.3 | − | +++
Cy5.5* | 1,069 | 1.44 | −4 | 680 | 697 | 21.0 | − | +++
CW800* | 1,091 | 2.51 | −4 | 786 | 800 | 14.2 | + | ++
ZW800-1 | 1,149 | −3.56 | 0 | 772 | 788 | 15.1 | +++ | −

*Carboxylic acid derivatives. Abbreviations: MB, methylene blue; ICG, indocyanine green; 800-CW, IRDye800-CW, NIRF, near-infrared fluorescent. For complete data, see Gioux et al. (6).

Table 2: Biodistribution of NIRF dyes CW800, RS800, ICG, ZW800-1, and ZW800-3a in mice and rats. Data are presented as CBR.

NIRF dye | Animal species | Organs
NIRF dye | Animal species | Kidneys | Muscle | Liver | Intestine | Rectum | Bladder
CW800 | Mouse | + | + | − | +++ | ++ | +++
CW800 | Rat | ++ | + | + | +++ | + | +++
RS800 | Mouse | + | − | − | ++ | +++ | ++
RS800 | Rat | + | − | − | +++ | ++ | −
ICG | Mouse | − | − | ++ | +++ | + | −
ICG | Rat | − | − | ++ | +++ | + | −
ZW800-1 | Mouse | − | − | − | − | − | +++
ZW800-1 | Rat | + | − | − | − | − | +++
ZW800-3a | Mouse | + | + | ++ | +++ | + | +++
ZW800-3a | Rat | ++ | ++ | +++ | ++ | − | +++

The contrast/background ratio (CBR) was calculated as (fluorescence signal − system background (BG))/BG. The CBR of each tissue was relative to the abdominal wall and was quantified as follows: −: 0 to 1; +: 1 to 2; ++: 2 to 5; and +++: >5. For complete data set, see Choi et al. (7)

Table 3: CBR, TBR, and PNR of tumors at 4 h p.i. in mice injected with cRGD-ZW800-1, cRGD-CW800, or cRGD-Cy5.5 (5).

cRGD-NIRF dye conjugate | TBR | | CBR | PNR
cRGD-NIRF dye conjugate | 4 h p.i. | 24 h p.i.* | CBR | PNR
ZW800-1 | 17.2 ± 1.2 | 4.8 | 5.1 ± 0.7 | 4.2 ± 0.9
CW800 | 5.1 ± 1.2 | 2.0 | 2.6 ± 0.2 | 2.1 ± 1.0
Cy5.5 | 2.7 ± 1.4 | 1.3 | 1.4 ± 0.2 | 1.4 ± 1.1

*Standard deviation not available. Abbreviations: TBR, CBR of tumor/CBR of surrounding normal tissues; PNR, CBR of receptor positive tumor/CBR of receptor negative tumor.